# ^99m^Tc-Cys-Gly-Gly-Affibody Z_HER2:342_

Chemical name: | ^99m^Tc-Cys-Gly-Gly-Affibody Z_HER2:342_
Abbreviated name: | ^99m^Tc-CGG-Z_HER2:342_
Synonym:
Agent category: | Antibody fragment, Affibody
Target: | EGF HER2 receptor
Target category: | Receptor
Method of detection: | SPECT, gamma planar
Source of signal: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=54792098), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?val=NM_201282.1) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=Graphics&list_uids=1956) for more information about HER2.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HER2%20342%20)]

Epidermal growth factor (EGF) is a cytokine that comprises 53 amino acids (6.2 kDa) and is secreted by ectodermic cells, monocytes, kidneys, and duodenal glands (1). EGF stimulates growth of epidermal and epithelial cells. EGF and at least seven other growth factors and their transmembrane receptor kinases play important roles in cell proliferation, survival, adhesion, migration, and differentiation. The EGF receptor (EGFR) family consists of four transmembrane receptors: EGFR (HER1/erbB-1), HER2 (erbB-2/neu), HER3 (erbB-3), and HER4 (erbB-4) (2). HER1, HER3, and HER4 comprise three major functional domains: an extracellular ligand-binding domain, a hydrophobic transmembrane domain, and a cytoplasmic tyrosine kinase domain. No ligand has been clearly identified for HER2. However, HER2 can be activated as a result of ligand binding to other HER receptors with the formation of receptor homodimers and/or heterodimers (3). HER1 and HER2 are overexpressed on many solid tumor cells such as breast, non-small cell lung, head and neck, and colon cancers (4-6). The high levels of HER1 and HER2 expression on cancer cells are associated with a poor prognosis (7-10).

Trastuzumab is a humanized IgG_1_ monoclonal antibody (mAb) against the extracellular domain of recombinant HER2 with an affinity constant (K_d_) of 0.1 nM (11). Trastuzumab is approved for clinical use for anti-cancer therapies in both Europe and North America. ^111^In-Trastuzumab, Cy5.5-trastuzumab, and ^68^Ga-trastuzumab-F(ab')_2_ eveloped for imaging human breast cancer (12-16). However, the pharmacokinetics of the intact radiolabeled mAb, with high liver uptake and slow blood elimination, are generally not ideal for imaging. Smaller antibody fragments, such as Fab or F(ab´)_2_, have better imaging pharmacokinetics because they are rapidly excreted by the kidneys. A novel class of recombinant affinity ligands (Affibody molecules) for HER2 was constructed on the basis of the Z-domain residues (58 amino acids) from one of the IgG-binding domains of staphylococcal protein A (17). Affibody molecules exhibit high binding affinity to HER2 with K_d_ values <100 pM. Various radiolabeled Affibody molecules have been studied in terms of their ability to image HER2 in tumors [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=affibody%20and%20HER2)]. Cys-Gly-Gly (CGG) was used a chelating linker for coupling ^99m^Tc to Z_HER2:342_ Affibody (18). ^99m^Tc-CGG-Z_HER2:342_ has been evaluated in nude mice bearing human SKOV-3 ovarian carcinoma xenografts.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HER2%20342%20and%20synthesis)]

Z_HER2:342_ Affibody was prepared by standard solid-phase peptide synthesis. CGG-Z_HER2:342_ was prepared by addition of CGG to the N-terminal of the Z-Affibody. ^99m^Tc as pertechnetate was added to a solution of CGG-Z_HER2:342_ containing SnCl_2_. The mixture was incubated for 60 min at room temperature. The labeling efficiency of ^99m^Tc incorporation was 94 ± 3% with >99% radiochemical purity. ^99m^Tc-CGG-Z_HER2:342_ was purified with size-exclusion chromatography. Specific activities of the preparations were not reported. ^99m^Tc-CGG-Z_HER2:342_ was found to be stable after incubation at 37°C for 2 h in saline buffer (91 ± 5%) or solution containing 300-fold excess cysteine (71 ± 6%).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HER2%20342%20and%20in%20vitro)]

Engfeldt et al. (18) performed binding experiments with CGG-Z_HER2:342_ with the use of a Biacore sensor chip immobilized with extracellular domain of HER2 protein. The K_d_ value of CGG-Z_HER2:342_ was calculated to be 280 pM. The K_d_ value of Z_HER2:342_ was 80 pM. Hence, the binding affinity of the synthetic Affibody molecule CGG-Z_HER2:342_ was 2.5-fold lower than the parent Affibody molecule Z_HER2:342_. In vitro binding specificity tests showed that binding of ^99m^Tc-CGG-Z_HER2:342_ to SKOV-3 cells expressing HER2 was receptor-mediated because saturation of receptors by preincubation with non-labeled Z_HER2:342_ significantly decreased binding of ^99m^Tc-CGG-Z_HER2:342_. The antigen binding capacity of ^99m^Tc-CGG-Z_HER2:342_ was 57 ± 2%. The cell-bound radioactivity remained constant at ~50% of the initially bound activity for up to 24 h when the cells were incubated with ^99m^Tc-CGG-Z_HER2:342_. In contrast, cells incubated with ^125^I-Z_HER2:342_ lost ~60% of the original cell-associated radioactivity.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HER2%20342%20and%20rodentia)]

Tran et al. (19) performed biodistribution studies of 0.1 MBq (2.7 μCi) ^99m^Tc-CGG3-Z_HER2:342_ in nude mice (n = 4) bearing SKOV-3 xenografts. ^99m^Tc-CGG-Z_HER2:342_ (0.14 nmol) was injected subcutaneously in each mouse. The initial tracer accumulation in the SKOV-3 tumors was 3.36% injected dose per gram (ID/g) at 1 h after injection, 4.23% ID/g at 4 h after injection, and 5.69% ID/g at 6 h after injection. The radioactivity level in tumors was higher at 6 h than in other organs and tissues except the kidneys (40% ID/g) and intestines (9.75% ID/g). The biodistribution was characterized by moderate clearance of radioactivity from blood and all organs and tissues. Blood levels were 2.32% ID/g at 2 h and 0.62% ID/g at 6 h. Tumor/muscle ratios were ~10, 18, and 35 at 1, 4, and 6 h after injection, respectively. Tumor/blood ratio was 9 at 6 h. Pre-administration of Z_HER2:342_ (83 nmol) decreased tumor accumulation from 4.23 ± 1.03 to 1.26 ± 0.14% ID/g (P = 0.05) at 4 h after injection. Biodistribution studies were also performed in normal NMRI mice (n = 4) without bearing any tumors at 4 h after injection. The results showed low accumulation in all organs and tissues except for the intestines (~12% ID/g) and the kidneys (50% ID/g). Single-photon emission computed tomography analysis was performed in nude mice (n = 2/group) bearing the SKOV-3 tumors after i.v. injection of 3 MBq (81 μCi) ^99m^Tc-CGG-Z_HER2:342_. Tumors were clearly visualized at 6 h along with the kidneys and abdomen area. Tumor/muscle ratio was 29 ± 7.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HER2%20342%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HER2%20342%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HER2%20342%20and%20human)]

No publication is currently available.

## References

1 Carpenter G., Cohen S. (1990). Epidermal growth factor. J Biol Chem.
2 Yarden Y. (2001). The EGFR family and its ligands in human cancer. signalling mechanisms and therapeutic opportunities. Eur J Cancer.
3 Rubin I., Yarden Y. (2001). The basic biology of HER2. Ann Oncol.
4 Grunwald V., Hidalgo M. (2003). Developing inhibitors of the epidermal growth factor receptor for cancer treatment. J Natl Cancer Inst.
5 Mendelsohn J. (1990). Anti-epidermal growth factor receptor monoclonal antibodies as potential anti-cancer agents. J Steroid Biochem Mol Biol.
6 Yasui W., Sumiyoshi H., Hata J., Kameda T., Ochiai A., Ito H., Tahara E. (1988). Expression of epidermal growth factor receptor in human gastric and colonic carcinomas. Cancer Res.
7 Ang K.K., Berkey B.A., Tu X., Zhang H.Z., Katz R., Hammond E.H., Fu K.K., Milas L. (2002). Impact of epidermal growth factor receptor expression on survival and pattern of relapse in patients with advanced head and neck carcinoma. Cancer Res.
8 Costa S., Stamm H., Almendral A., Ludwig H., Wyss R., Fabbro D., Ernst A., Takahashi A., Eppenberger U. (1988). Predictive value of EGF receptor in breast cancer. Lancet.
9 Ethier S.P. (1995). Growth factor synthesis and human breast cancer progression. J Natl Cancer Inst.
10 Yarden Y. (2001). Biology of HER2 and its importance in breast cancer. Oncology.
11 Carter P., Presta L., Gorman C.M., Ridgway J.B., Henner D., Wong W.L., Rowland A.M., Kotts C., Carver M.E., Shepard H.M. (1992). Humanization of an anti-p185HER2 antibody for human cancer therapy. Proc Natl Acad Sci U S A.
12 Perik P.J., Lub-De Hooge M.N., Gietema J.A., van der Graaf W.T., de Korte M.A., Jonkman S., Kosterink J.G., van Veldhuisen D.J., Sleijfer D.T., Jager P.L., de Vries E.G. (2006). Indium-111-labeled trastuzumab scintigraphy in patients with human epidermal growth factor receptor 2-positive metastatic breast cancer. J Clin Oncol.
13 Lub-de Hooge M.N., Kosterink J.G., Perik P.J., Nijnuis H., Tran L., Bart J., Suurmeijer A.J., de Jong S., Jager P.L., de Vries E.G. (2004). Preclinical characterisation of 111In-DTPA-trastuzumab. Br J Pharmacol.
14 Garmestani K., Milenic D.E., Plascjak P.S., Brechbiel M.W. (2002). A new and convenient method for purification of 86Y using a Sr(II) selective resin and comparison of biodistribution of 86Y and 111In labeled Herceptin. Nucl Med Biol.
15 Smith-Jones P.M., Solit D., Afroze F., Rosen N., Larson S.M. (2006). Early tumor response to Hsp90 therapy using HER2 PET: comparison with 18F-FDG PET. J Nucl Med.
16 Smith-Jones P.M., Solit D.B., Akhurst T., Afroze F., Rosen N., Larson S.M. (2004). Imaging the pharmacodynamics of HER2 degradation in response to Hsp90 inhibitors. Nat Biotechnol.
17 Wikman M., Steffen A.C., Gunneriusson E., Tolmachev V., Adams G.P., Carlsson J., Stahl S. (2004). Selection and characterization of HER2/neu-binding affibody ligands. Protein Eng Des Sel.
18 Engfeldt, T., A. Orlova, T. Tran, A. Bruskin, C. Widstrom, A.E. Karlstrom, and V. Tolmachev, Imaging of HER2-expressing tumours using a synthetic Affibody molecule containing the (99m)Tc-chelating mercaptoacetyl-glycyl-glycyl-glycyl (MAG3) sequence. Eur J Nucl Med Mol Imaging, 2006
19 Tran T., Engfeldt T., Orlova A., Widstrom C., Bruskin A., Tolmachev V., Karlstrom A.E. (2007). In vivo evaluation of cysteine-based chelators for attachment of 99mTc to tumor-targeting Affibody molecules. Bioconjug Chem.